# Microbubbles conjugated with cyclo(CGGRRLGGC)

Chemical name: | Microbubbles conjugated with cyclo(CGGRRLGGC)
Abbreviated name: | MB_RRL_
Synonym:
Agent Category: | Peptide
Target: | Unknown
Target Category: | Receptor binding to tumor-derived endothelial cells
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL)]

Ultrasound is the most widely used imaging modality (1), and its role in non-invasive molecular imaging is expanding with ligand-carrying microbubbles (2). Microbubbles are spherical cavities filled with a gas encapsulated in a shell. The shells are made of phospholipids, a surfactant, denatured human serum albumin, or a synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles, which are usually 2–8 μm in diameter. Microbubbles provide a strongly reflective interface and resonate to ultrasound waves, and they are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They also have the potential to be used for drug and gene delivery (6).

Endothelial cells are important cells in inflammatory responses (7, 8). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α, interleukin-1, and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on the leukocytes rolling along endothelial cell surfaces and subsequently adhering to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1, integrins, and selectins. Chemokines are chemotactic to leukocytes at sites of inflammation and tissue injury (9). Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels. Tumor growth depends on the formation of new blood vessels from angiogenesis. Vascular endothelial growth factor (VEGF) and basic fibroblast growth factor (bFGF) enhance angiogenesis. Expression of VEGF receptors is higher on the cell surface of tumor-derived endothelial cells than on the cell surface of normal endothelial cells.

Microbubbles conjugated to peptides or to antibodies against integrins, cell adhesion molecules, and VEGF receptors have previously been studied for the non-invasive assessment and imaging of angiogenesis (10-13). A peptide specific to tumor vasculature and containing Arg-Arg-Leu (RRL) was identified by screening a peptide display library panned against tumor cells derived from SCC-VII murine squamous cell carcinomas (14). Weller et al. (12) studied ultrasonic imaging of tumor vasculature using microbubbles conjugated with biotinylated c(CGGRRLGGC) (MB_RRL_) in mice bearing human tumor xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20synthesis)]

For targeted microbubbles, Weller et al. (12) prepared biotinylated microbubbles by sonication of an aqueous dispersion of decafluorobutane gas, phosphatidylcholine, polyethylene glycol-stearate, and phosphatidylethanolamine-biotin in a 2:1:1 ratio by weight. Microbubbles were combined with streptavidin, washed, and conjugated with MB_RRL_ or control peptide c(CGGGGGGGC) (MB_control_). The microbubbles are 3.2 ± 1.0 μm in diameter. The peptide/microbubble ratio was estimated with flow cytometry to be ~60,000 (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20in%20vitro)]

Weller et al. (12) reported that MB_RRL_ or MB_control_ (3.33 × 10^6^/ml) perfused through the flow chamber coated with endothelial cells at a wall shear rate of 100 s^-1^ for 3 min. There was a significantly (P < 0.01) greater number of MB_RRL_ attached to tumor-activated endothelial cells (2.4 ± 0.6 microbubbles/cell) than to normal endothelial cells (0.8 ± 0.1 microbubbles/cell). MB_control_ attachment to both activated and normal endothelial cells was minimal (0.3–0.4 microbubbles/cell).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20rodentia)]

Weller et al. (12) performed ultrasound assessment of MB_RRL_ binding in five mice bearing Clone C tumors (transfected with bFGF), six mice bearing PC3 tumors, and six normal mice. There were intense acoustic signals in both tumors at 2 min after MB_RRL_ injection compared with mild contrast in tumors injected with MB_control_. There was little difference in myocardial signal intensity between MB_RRL_ and MB_control_ in normal mice. The mean video intensity for normal myocardium was 0.5 ± 1 units, whereas the mean video intensity for the tumors was 5 ± 1 units (P = 0.0001). Postmortem histology demonstrated that the density of RRL binding was concentrated at the tumor periphery. No blocking studies or other studies to validate the mechanism were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20RRL%20and%20human)]

No publication is currently available.

## NIH Support

R01 HL-58865

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2. Liang, H.D. and M.J. Blomley, The role of ultrasound in molecular imaging. Br J Radiol, 2003. 76 Spec No 2: p. S140-50.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
8 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
9 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
10 Villanueva F.S., Jankowski R.J., Klibanov S., Pina M.L., Alber S.M., Watkins S.C., Brandenburger G.H., Wagner W.R. (1998). Microbubbles targeted to intercellular adhesion molecule-1 bind to activated coronary artery endothelial cells. Circulation.
11 Weller G.E., Lu E., Csikari M.M., Klibanov A.L., Fischer D., Wagner W.R., Villanueva F.S. (2003). Ultrasound imaging of acute cardiac transplant rejection with microbubbles targeted to intercellular adhesion molecule-1. Circulation.
12 Weller G.E., Villanueva F.S., Klibanov A.L., Wagner W.R. (2002). Modulating targeted adhesion of an ultrasound contrast agent to dysfunctional endothelium. Ann Biomed Eng.
13 Reinhardt M., Hauff P., Linker R.A., Briel A., Gold R., Rieckmann P., Becker G., Toyka K.V., Maurer M., Schirner M. (2005). Ultrasound derived imaging and quantification of cell adhesion molecules in experimental autoimmune encephalomyelitis (EAE) by Sensitive Particle Acoustic Quantification (SPAQ). Neuroimage.
14 Brown C.K., Modzelewski R.A., Johnson C.S., Wong M.K. (2000). A novel approach for the identification of unique tumor vasculature binding peptides using an E. coli peptide display library. Ann Surg Oncol.